# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-cyclo(D-diaminobutyric acid-Arg-Phe-Phe-D-Trp-Lys-Thr-Phe)

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-cyclo(D-diaminobutyric acid-Arg-Phe-Phe-D-Trp-Lys-Thr-Phe)
Abbreviated name: | ^111^In-KE88, ^111^In-DOTA-cyclo(dDab-RFFwKTF)
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptors (SSRs)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_–sst_5_) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Labeled diethylenetriaminepentaacetic acid-octreotide ((^111^In-DTPA-OCT) is an SSTR analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (5). It has also showed promising results in peptide-receptor radionuclide therapy (6). ^111^In-DTPA-OCT binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree, but it does not bind to sst_1_ or sst_4_ (7). Currently used targeting SSTR peptides mainly have affinity for sst_2_. However, sst_1_, sst_3_, sst_4_, and sst_5_ are also expressed in different tumors. Therefore, there is a need for pansomatostatin radioligands (8). Ginj et al. (9) has developed a series of pansomatostatin ligands. One of them, 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-cyclo(D-diaminobutyric acid-Arg-Phe-Phe-D-Trp-Lys-Thr-Phe) (KE88) was found to be an agonist to all sst subtypes. For evaluation as a SPECT imaging agent for all sst subtypes, ^111^In has been attached to KE88 via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^111^In-KE88.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88+and+synthesis)]

DOTA-tris(tert-butylester) was used to conjugate the N-terminal amino acid to form KE88 after standard solid-phase peptide synthesis of KE88 (9). KE88 was purified with high-performance liquid chromatography. ^111^InCl_3_ was conjugated to KE88 with a radiochemical yield of >95%. ^111^In-KE88 had a >97% radiochemical purity and a specific activity of ~37 GBq/µmol (1 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88+and+in+vitro)]

Ginj et al. (9) showed that KE88 exhibited an agonistic effect on forskolin-stimulated cAMP accumulation in CCL39 cells expressing sst_1_–sst_5_ with effective concentrations of 7.35, 9.73, 1.92, 0.47, and 2.66 nM, respectively. ^111^In-KE88 internalization into HEK-sst_2_, HEK-sst_3_, and HEK-sst_5_ cells was performed after 4 h of incubation at 37°C with <0.5, 32.2, and <0.1%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88+and+rodentia)]

Ginj et al. (9) performed ex vivo biodistribution studies with ^111^In-KE88 in nude mice (n = 3/group) bearing xenografts of HEK-sst_2_ tumor cells on one flank and HEK-sst_3_ tumors on the other flank. The accumulation of ^111^In-KE88 in the HEK-sst_3_ tumors was 15.2% injected dose per gram (% ID/g) at 15 min, 22.9% ID/g at 1 h, 23.2% ID/g at 4 h, and 14.9% ID/g at 24 h after injection, whereas the accumulation in the HEK-sst_2_ tumors was 18.5, 13.6, 3.7, and 1.1% ID/g at the time points, respectively. Therefore, the sst_3_ tumors exhibited a higher ^111^In-KE88 accumulation and slower washout than the sst_2_ tumors. The kidney was the only organ that had a higher accumulation at 1 h after injection than the tumors with 64% ID/g, followed by the pituitary (9% ID/g) and liver (2.7% ID/g). Accumulation of radioactivity in the other tissues was low at I h after injection. The concentration in the blood was only 0.1% ID/g at 4 h after injection, with tumor/blood ratios of 232 for the sst_3_ tumors and 37 for the sst_2_ tumors. Co-injection with DOTA-TATE (sst_2_-selective ligand) reduced the accumulation of the radioactivity by 90% in the sst_2_ tumors at 1 h after injection. Co-injection with ^111^In-DTPA-TATE and KE88 reduced the accumulation of the radioactivity by 84% in the sst_3_ tumors. Whole-body SPECT imaging visualized the sst_3_ tumor as early as 1 h after ^111^In-KE88 injection with a strong radioactivity signal in the kidneys. In contrast, the sst_2_ tumor was barely visualized. By 4 h, only the sst_3_ tumor and kidneys were visible.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=KE88+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
6 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
7 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
8 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
9 Ginj M., Zhang H., Eisenwiener K.P., Wild D., Schulz S., Rink H., Cescato R., Reubi J.C., Maecke H.R. (2008). New pansomatostatin ligands and their chelated versions: affinity profile, agonist activity, internalization, and tumor targeting. Clin Cancer Res.